# ^64^Cu-Anti-human integrin α_v_β_3_ monoclonal antibody

Chemical name: | ^64^Cu-Anti-human integrin α_v_β_3_ monoclonal antibody
Abbreviated name: | ^64^Cu-DOTA-hLM609-II
Synonym: | ^64^Cu-Abegrin™, ^64^Cu-Vitaxin™, ^64^Cu-MEDI522™, ^64^Cu-LM609, ^64^Cu-anti- α_v_β_3_ MAb
Agent Category: | Antibody
Target: | Integrin α_v_β_3_
Target Category: | Antibody-antigen binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29)]

^64^Cu-Anti-human integrin α_v_β_3_ monoclonal antibody (^64^Cu-DOTA-hLM609-II) is a radiolabeled antibody developed for positron emission tomography (PET) imaging of integrin α_v_β_3_−positive tumors (1). ^64^Cu-DOTA-hLM609-II is labeled with ^64^Cu which is a positron emitter with a half-life (t_½_) of 12.7 h.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiological processes. Among the molecules that regulate angiogenesis are integrins, a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (2, 3).These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. The integrin α_v_β_3_ receptor is generally not found in normal tissue but is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Increased levels of integrin α_v_β_3_ expression are closely associated with increased cell invasion and metastasis. Molecular imaging of a probe that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (4, 5).

Radiolabeled monoclonal antibodies (MAbs) have been developed for both the diagnosis and treatment of tumors (6-8). Radiometals with appropriate photon or positron emissions can be used to radiolabel antibodies and in imaging studies (9, 10). Cheresh and Harper (11, 12) first reported the synthesis of LM609 MAb, a murine IgG1 antibody (mLM609), which appeared to react with and recognize α_v_β_3_ as one entity. The mLM609 was humanized by grafting the murine complementary-determining regions (CDRs) onto a human framework (13, 14). The humanized LM609 (hLM609) was shown to retain the affinity properties of the murine antibody. This first version of hLM609 (hLM609-I) was used in clinical studies (http://clinicaltrials.gov/ct2/results?term=MEDI522) for cancer therapy (15). These studies reported no significant toxicity or immune response from hLM609-I. However, ^99m^Tc labeling of hLM609-I was unsuccessful due to the in vivo instability of the ^99m^Tc label (16). Another clone (hLM609-II) with >50-fold enhanced affinity was also produced using a phage-expressed libraries and focused mutagenesis strategy in a stepwise fashion (13, 15). hLM609-II is currently in clinical trials for treatment of prostate cancer, psoriasis, melanoma, and rheumatoid arthritis. Cai et al. (1) successfully radiolabeled hLM609-II with ^64^Cu using 1,4,7,10-tetra-azacyclododecane N,N',N'',N'''-tetraacetic acid (DOTA) as the bifunctional chelator.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20synthesis)]

Cheresh et al. (11, 15) used the standard hybridoma technique to produce murine mLM609 MAb against the M21 human melanoma cell adhesion receptor. mLM609 specifically blocked endothelial cell attachment to von Willebrand factor, fibrinogen, vitronectin, and an RGD peptide. mLM609-I was humanized by phage expression technologies and codon-based mutagenesis (13, 14). This hLM609 retained the properties of mLM609 as determined by in vitro and in vivo characterization. Wu et al. (13) improved the binding characteristics of hLM609-I by constructing phage-expressed libraries of hLM609-I Fab variants and a mutagenesis strategy that mutated every position of all six CDRs. The expression and screening of a combinatorial library produced 2592 variants. This resulted in obtaining the hLM609-II clone that displayed >50-fold enhanced affinity. Cai et al. (1) used DOTA to conjugate and radiolabel hML609-II. Briefly, commercially obtained DOTA was activated by 1-ethyl-3-[3-(dimethylamino)-propyl] carbodimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) at pH 5.5 for 30 min with a molar ratio of 10:5:4 (DOTA:EDC:SNHS). The activated product, DOTA-N-hydroxysulfosuccinimidyl, was cooled to 4°C and added to hLM609-II. The mixture was adjusted to pH 8.5 and allowed to incubate for overnight at 4°C. In the radiolabeling, ^64^Cu chloride (^64^CuCl_2_) was diluted in 300 µl of 0.1 mol/liter sodium acetate buffer (pH 6.5) and added to the DOTA-hLM609-II conjugates in a ratio of 25 µg DOTA-hLM609-II per mCi of ^64^Cu. The reaction mixture was incubated for 1 h at 40°C. ^64^Cu-DOTA-hLM609-II was purified by PD-10 column. Radiolabeling yields appeared to be dependent on the DOTA/hLM609-II ratios in the reaction mixtures. The % yields (n = 3) were 5.20 ± 3.16 (20:1), 14.05 ± 17.12 (50:1), 25.32 ± 11.50 (100:1), 37.32 ± 25.94 (200:1), and 88.12 ± 6.98 (1000:1). The average numbers of DOTA per hLM609-II molecule were calculated as 1.65 ± 0.32 (20:1), 3.29 ± 2.01 (50:1), 6.38 ± 3.52 (100:1), 9.20 ± 3.16 (200:1), and 38.53 ± 5.71 (1000:1). The specific activities varied from 78.07 ± 47.36 MBq/mg (2.11 ± 1.28 mCi/mg) to 957.93 ± 75.85 MBq/mg (25.89 ± 2.05 mCi/mg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20in%20vitro)]

The immunoreactivity of each ^64^Cu-DOTA-hLM609-II preparation from different DOTA/hLM609-II ratios was tested by binding assay with integrin α_v_β_3_−positive U87MG cells (1). Regardless of the DOTA/hLM609-II ratios and yields, all preparations (n = 3) had similar immunoreactivity which ranged from 59.78 ± 1.33% to 71.13 ± 2.58%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20rodentia)]

Biodistribution studies of ^64^Cu-DOTA-hLM609-II were conducted in nude mice bearing MDA-MB-435 human breast tumors (1). Each mouse received 0.74 MBq (20 µCi) of ^64^Cu-DOTA-hLM609-II. All ^64^Cu-DOTA-hLM609 preparations with different DOTA/hLM609-II ratios showed good tumor radioactivity levels. The 1000:1 DOTA/hLM609-II ratio preparation (n = 3) had the highest tumor radioactivity uptakes expressed in percentage injected dose/g (% ID/g) with 12.50 ± 2.73 (4 h), 39.88 ± 7.05 (25 h), and 49.41 ± 4.54 (71 h). High radioactivity levels were also found in the heart and liver at early time points, which then dropped steadily over time. The radioactivity levels (% ID/g) in the heart were 29.08 ± 5.90 (4 h), 13.89 ± 3.13 (17 h), and 4.38 ± 0.28 (71 h). The radioactivity levels in the liver were 19.56 ± 4.43 (4 h), 11.91 ± 1.68 (17 h), and 8.51 ± 1.31 (71 h). The serum t_½_ was ~12−24 h.

The 1000:1 DOTA/hLM609-II ratio preparation was used in PET imaging of mouse tumor models with different integrin α_v_β_3_ cell density levels in the following order: U87MG human glioblastoma > MDA-MB-435 human breast carcinoma > PC-3 human prostate adenocarcinoma ~GL-26 mouse glioblastoma (1). Each mouse received 7.4−11.1 MBq (200-300 µCi) ^64^Cu-DOTA-hLM609-II radioactivity. All tumors exhibited high tumor activity by 17 h after injection and increased over time. The tumor signal intensity was highest with U87MG, whereas the signals for MDA-MB-435 and PC-3 were similar. The GL-26 mouse glioblastoma signal intensity reached a peak at 24 h and then steadily dropped over time. The authors suggested that this low activity uptake in mouse tumor was because hLM609-II did not cross-reacted with mouse integrin α_v_β_3_. Blocking studies with coinjection of 2 mg of unlabeled hLM609-II showed effective blocking of 50-65% ^64^Cu-DOTA-hLM609-II radioactivity uptake in mice bearing MDA-MB-435 tumors (extrapolated from Figure 5A).

Immunofluorescence staining was performed in tumor sections after PET imaging studies with ^64^Cu-DOTA-hLM609-II (1). These ex vivo experiments confirmed the human integrin α_v_β_3_− specific binding of ^64^Cu-DOTA-hLM609-II.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2864Cu-Labeled%20Abegrin%29%20OR%20%28Anti-integrin%20monoclonal%20antibody%29%29%20AND%20human)]

Based on PET imaging data from rats, Cai et al. (1) estimated human absorbed doses (n = 3) of ^64^Cu-DOTA-hLM609-II to normal organs. The rat organ distribution of ^64^Cu-DOTA-hLM609-II was similar to that of mice with the exception that the liver radioactivity level was more prominent and persistent. The liver appeared to be the critical organ with 0.330 ± 0.020 mGy/MBq (1.220 ± 0.076 rad/mCi). The estimated radiation absorbed doses (mGy/MBq) in other major organs of an adult human were 0.207 ± 0.011 in the spleen (0.766 ± 0.040 rad/mCi), 0.044 ± 0.001 in the gallbladder (0.163 ± 0.004 rad/mCi ), 0.060 ± 0.002 in the heart: (0.221 ± 0.009 rad/mCi), 0.036 ± 0.003 in the kidneys (0.132 ± 0.012 rad/mCi), 0.032 ± 0.000 in the adrenals (0.117 ± 0.001 rad/mCi), 0.032 ± 0.000 in the pancreas (0.117 ± 0.001 rad/mCi), and 0.015 ± 0.001 in the brain (0.117 ± 0.001 rad/mCi ), The whole-body effective dose was 0.034 ± 0.001 mGy/MBq (0.127 ± 0.003 rad/mCi).

## NIH Support

NIH NIBIB R21 EB001785, NCI R21CA102123, NCI In Vivo Cellular Molecular Imaging Center grant P50 CA114747, NCI Small Animal Imaging Resource Program grant R24 CA93862, NCI Centers of Cancer Nanotechnology Excellence U54 grant IU54CA119367-01. NIH CA42508-01.

## References

1 Cai W., Wu Y., Chen K., Cao Q., Tice D.A., Chen X. (2006). In vitro and In vivo Characterization of 64Cu-Labeled AbegrinTM, a Humanized Monoclonal Antibody against Integrin {alpha}v{beta}3. Cancer Res.
2 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
3 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
4 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
5 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
6 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
7 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
8 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
9 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
10 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.
11 Cheresh D.A. (1987). Human endothelial cells synthesize and express an Arg-Gly-Asp-directed adhesion receptor involved in attachment to fibrinogen and von Willebrand factor. Proc Natl Acad Sci U S A.
12 Cheresh D.A., Harper J.R. (1987). Arg-Gly-Asp recognition by a cell adhesion receptor requires its 130-kDa alpha subunit. J Biol Chem.
13 Wu H., Beuerlein G., Nie Y., Smith H., Lee B.A., Hensler M., Huse W.D., Watkins J.D. (1998). Stepwise in vitro affinity maturation of Vitaxin, an alphav beta3-specific humanized mAb. Proc Natl Acad Sci U S A.
14 Rosok M.J., Yelton D.E., Harris L.J., Bajorath J., Hellstrom K.E., Hellstrom I., Cruz G.A., Kristensson K., Lin H., Huse W.D., Glaser S.M. (1996). A combinatorial library strategy for the rapid humanization of anticarcinoma BR96 Fab. J Biol Chem.
15 Cai W., Chen X. (2006). Anti-angiogenic cancer therapy based on integrin alphavbeta3 antagonism. Anticancer Agents Med Chem.
16 Posey J.A., Khazaeli M.B., DelGrosso A., Saleh M.N., Lin C.Y., Huse W., LoBuglio A.F. (2001). A pilot trial of Vitaxin, a humanized anti-vitronectin receptor (anti alpha v beta 3) antibody in patients with metastatic cancer. Cancer Biother Radiopharm.